# ^64^Cu-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-MEDI-522

Chemical name: | ^64^Cu-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-MEDI-522
Abbreviated name: | ^64^Cu-DOTA-MEDI-522
Synonym: | ^64^Cu-DOTA-Abegrin, ^64^Cu-DOTA-Vitaxin
Agent category: | Antibody
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MEDI-522)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents, and the agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (inhibition concentration (IC_50_), 7–40 nM) but not to integrins α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM). Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). In addition to RGD peptides, a humanized anti-human integrin α_v_β_3_ monoclonal antibody (MEDI-522) was identified to be unique in that it recognizes either the human α_v_ or β_3_ subunit. MEDI-522 cross-reacts with integrin α_v_β_3_ from rabbits, chickens, and hamsters but not with integrin α_v_β_3_ from mice or rats (13). MEDI-522 is being evaluated as an antiangiogenic agent for cancer therapy (14-16). Cai et al. (17) reported the development of ^64^Cu-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-MEDI-522 (^64^Cu-DOTA-MEDI-522) for positron emission tomography (PET) imaging of α_v_β_3_ receptors in nude mice bearing tumors.

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD), MEDI-522 (http://www.clinicaltrials.gov/ct2/results?term=MEDI-522))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20MEDI-522+synthesis)]

DOTA was incubated with EDC and SNHS for 30 min at pH 5.5 with a molar ratio of 10:5:4 (17). The product, DOTA-N-hydroxysulfosuccinimidyl (DOTA-OSSu), was added to MEDI-522 in a molar ratio of 1,000:1 (DOTA-OSSu/MEDI-522). The reaction mixture was adjusted to pH 8.5 and incubated for ~18 h at 4°C. DOTA-MEDI-522 was purified with column chromatography. DOTA-MEDI-522 (0.33 nmol) was incubated with 74 MBq (2 mCi) ^64^CuCl_2_ in sodium acetate buffer (pH 6.5) for 1 h at 40°C. ^64^Cu-DOTA-MEDI-522 was purified with column chromatography. This procedure provided a radiolabeling yield of 88% with a specific activity of 148 MBq/nmol (4 mCi/nmol). There were ~39 DOTA moieties per ^64^Cu-DOTA-MEDI-522. The immunoreactivity was determined to be 63% with integrin α_v_β_3_-positive U87MG human glioblastoma cells. Control ^64^Cu-DOTA-IgG was prepared similarly. Decreasing the DOTA-OSSu/MEDI-522 molar ratios to 200:1 and 100:1 yielded final labeled ^64^Cu-DOTA-MEDI-522 conjugates that contained 10 and 6 DOTA moieties, respectively, with similar immunoreactivity.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20MEDI-522%20in+vitro)]

Liu et al. (18) performed saturation binding studies of ^125^I-MEDI-522 on U87MG cells. ^125^I-MEDI-522 showed a K_d_ value (affinity constant) of 0.35 ± 0.06 nM and a B_max_ value (receptor density) of 2.5 × 10^5^ sites per cell. MEDI-522 and DOTA-MEDI-522 exhibited an inhibition curve similar to that of ^125^I-MEDI-522 binding to U87MG cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20MEDI-522+rodentia)]

Cai et al. (17) performed PET and ex vivo biodistribution studies of ^64^Cu-DOTA-MEDI-522 in nude mice (n = 3/group) bearing MDA-MB-435 human breast carcinoma tumors at 18 h and 46 h after injection. Ex vivo tumor accumulation was 4.54 ± 0.39% injected dose/gram (ID/g) and 5.40 ± 0.75% ID/g at 18 h and 44 h after injection, respectively. PET imaging revealed estimated tumor accumulation values of 5.63 ± 1.16% injected dose/gram (ID/g) and 7.04 ± 1.47% at 18 h and 46 h after injection, respectively. There was no significant difference between the two methods of measurement (P = 0.16). Accumulation in the liver and spleen was approximately two-fold higher than in the tumor. The other normal tissues showed less accumulation than the tumor. Co-injection of excess MEDI-522 inhibited tumor accumulation by ~70% at 46 h after injection as measured with PET imaging.

Another PET imaging study was performed with mice (n = 3/group) bearing tumors with different α_v_β_3_ expression levels. U87MG tumor cells showed higher signal at 17–71 h after injection than MDA-MB-435 cells, GL-26 mouse glioblastoma, and PC-3 human prostate adenocarcinoma tumors, agreeing with their degree of human α_v_β_3_ expression. Immunofluorescence staining of tumor sections confirmed MEDI-522 binding in human tumor cells but not in mouse tumor cells or in mouse tumor vasculature because MEDI-522 does not cross-react with mouse β_3_. Anti-mouse β_3_ antibody binding was observed only in mouse tumor cells and mouse tumor vasculature.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20MEDI-522+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20MEDI-522+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20MEDI-522+human)]

No publication is currently available.

## NIH Support

R21 EB001785, R21 CA102123, P50 CA114747, R24 CA93862, 1U54 CA119367-01

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Wu H., Beuerlein G., Nie Y., Smith H., Lee B.A., Hensler M., Huse W.D., Watkins J.D. (1998). Stepwise in vitro affinity maturation of Vitaxin, an alphav beta3-specific humanized mAb. Proc Natl Acad Sci U S A.
14 McNeel D.G., Eickhoff J., Lee F.T., King D.M., Alberti D., Thomas J.P., Friedl A., Kolesar J., Marnocha R., Volkman J., Zhang J., Hammershaimb L., Zwiebel J.A., Wilding G. (2005). Phase I trial of a monoclonal antibody specific for alphavbeta3 integrin (MEDI-522) in patients with advanced malignancies, including an assessment of effect on tumor perfusion. Clin Cancer Res.
15 Posey J.A., Khazaeli M.B., DelGrosso A., Saleh M.N., Lin C.Y., Huse W., LoBuglio A.F. (2001). A pilot trial of Vitaxin, a humanized anti-vitronectin receptor (anti alpha v beta 3) antibody in patients with metastatic cancer. Cancer Biother Radiopharm.
16 Gutheil J.C., Campbell T.N., Pierce P.R., Watkins J.D., Huse W.D., Bodkin D.J., Cheresh D.A. (2000). Targeted antiangiogenic therapy for cancer using Vitaxin: a humanized monoclonal antibody to the integrin alphavbeta3. Clin Cancer Res.
17 Cai W., Wu Y., Chen K., Cao Q., Tice D.A., Chen X. (2006). In vitro and in vivo characterization of 64Cu-labeled Abegrin, a humanized monoclonal antibody against integrin alpha v beta 3. Cancer Res.
18 Liu Z., Jia B., Zhao H., Chen X., Wang F. (2011). Specific targeting of human integrin alpha(v)beta (3) with (111)In-labeled Abegrin in nude mouse models. Mol Imaging Biol.